# ^64^Cu-Polyethylenimine

Chemical name: | ^64^Cu-Polyethylenimine
Abbreviated name: | ^64^Cu-PEI
Synonym:
Agent category: | Compound
Target: | Heparin sulfate proteoglycans
Target category: | Other
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine)]

Polyethylenimine (PEI) is an organic polymer with a high density of amino groups that can be protonated. At physiological pH, the positively charged PEI binds to DNA as a gene carrier (1). PEI binds to negatively charged heparin sulfate proteoglycans on the cell surface, thus facilitating the transfection of eukaryotic cells (2). Currently, [^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG) (3) and ^64^Cu-pyruvaldehyde-bis(N^4^-methylthiosemicarbazone) (^64^Cu-PTSM) (4) have been studied as positron emission tomography (PET) cell-trafficking agents. However, studies of FDG-labeled cells were limited to ~6 h because of the short physical half-life of ^18^F (110 min). Li et al. (5) labeled PEI with ^64^Cu without using a metal chelator. ^64^Cu-PEI was evaluated as a tumor-imaging probe and as a cell-labeling agent for cell trafficking in comparison to ^64^Cu-PTSM.

### Related Resource Links:

- Chapters in MICAD (FDG (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FDG), PTSM (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Cu-PTSM))
- Clinical trials (Polyethylenimine (http://www.clinicaltrials.gov/ct2/results?term=Polyethylenimine))
- FDA Drug information (Polyethylenimine (http://google2.fda.gov/search?q=Polyethylenimine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+synthesis)]

PEI (0.8 nmol) and ^64^CuCl_2_ (74 MBq (2 mCi)) were mixed in sodium acetate buffer (pH, 6.5) for 1 h at 40°C (5). ^64^Cu-PEI was purified on a PD-10 column. The labeling yield was >90%, and the specific activity was >80 GBq/µmol (2.2 Ci/µmol). In comparison, the specific activity for ^64^Cu-PTSM was 1.8 GBq/µmol (48.6 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+in+vitro)]

Li et al. (5) performed in vitro uptake and efflux studies of ^64^Cu-PEI and ^64^Cu-PTSM in cultured U87MG human glioblastoma cells. ^64^Cu-PEI and ^64^Cu-PTSM exhibited 20% and 60% uptake of incubation dose within 90 min of incubation at 37°C, respectively. ^64^Cu-PTSM exhibited a lower efflux (36% at 27 h) than ^64^Cu-PEI (61% at 27 h). Therefore, ^64^Cu-PTSM would be a better cell-labeling agent for cell trafficking than ^64^Cu-PEI.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+%20rodentia)]

Li et al. (5) performed ex vivo biodistribution studies in mice (n = 3/group) bearing U87MG tumors at 48 h after injection of ^64^Cu-PEI. The liver, tumor, and kidney accumulations were 15%, 13%, and 10% injected dose per gram (ID/g), respectively. The intestine, lung, heart, spleen, muscle, pancreas, blood, and brain had lower accumulation than the kidneys. PET imaging was performed in mice (n = 3/group) bearing U87MG tumors at 48 h after injection of 7.2 MBq (0.2 mCi) ^64^Cu-PEI or ^64^Cu-PTSM. For ^64^Cu-PEI, the tumor accumulation was 11.0 ± 3.8, 17.4 ± 3.3, and 18.7 ± 2.2% ID/g at 1, 4, and 24 h after injection, respectively. For ^64^Cu-PTSM, the tumor accumulation was 12.5 ± 1.7, 13.6 ± 0.8, and 12.4 ± 1.7% ID/g at 1, 4, and 24 h after injection, respectively. Both tracers exhibited similar high liver radioactivity, whereas ^64^Cu-PTSM exhibited a higher kidney accumulation than ^64^Cu-PEI. The accumulation of ^64^Cu-PTSM in the brain was as high as that in the tumors, whereas little radioactivity was observed with ^64^Cu-PEI in the brain. In another PET experiment, U87MG tumor cells labeled with ^64^Cu-PEI or ^64^Cu-PTSM were injected intravenously in mice. Both ^64^Cu-PEI- and ^64^Cu-PTSM-labeled cells were found in the lungs at 5 min after injection and were redistributed in similar proportions to the kidneys and liver at later time points (up to 4 h).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu%20polyethyleneimine+human)]

No publication is currently available.

## NIH Support

R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Jere D., Jiang H.L., Arote R., Kim Y.K., Choi Y.J., Cho M.H., Akaike T., Cho C.S. (2009). Degradable polyethylenimines as DNA and small interfering RNA carriers. Expert Opin Drug Deliv.
2 Suk J.S., Suh J., Choy K., Lai S.K., Fu J., Hanes J. (2006). Gene delivery to differentiated neurotypic cells with RGD and HIV Tat peptide functionalized polymeric nanoparticles. Biomaterials.
3 Doyle B., Kemp B.J., Chareonthaitawee P., Reed C., Schmeckpeper J., Sorajja P., Russell S., Araoz P., Riederer S.J., Caplice N.M. (2007). Dynamic tracking during intracoronary injection of 18F-FDG-labeled progenitor cell therapy for acute myocardial infarction. J Nucl Med.
4 Adonai N., Nguyen K.N., Walsh J., Iyer M., Toyokuni T., Phelps M.E., McCarthy T., McCarthy D.W., Gambhir S.S. (2002). Ex vivo cell labeling with 64Cu-pyruvaldehyde-bis(N4-methylthiosemicarbazone) for imaging cell trafficking in mice with positron-emission tomography. Proc Natl Acad Sci U S A.
5 Li Z.B., Chen K., Wu Z., Wang H., Niu G., Chen X. (2009). 64Cu-labeled PEGylated polyethylenimine for cell trafficking and tumor imaging. Mol Imaging Biol.